# Indotricarbocyanine-loaded AS1411 DNA aptamer- and TGN peptide-modified poly(ethylene glycol)-poly(ε-caprolactone) nanoparticles

Chemical name: | Indotricarbocyanine-loaded AS1411 DNA aptamer- and TGN peptide-modified poly(ethylene glycol)-poly(ε-caprolactone) nanoparticles
Abbreviated name: | DiR-AsTNP
Synonym: | AsTNP
Agent Category: | Nanoparticles
Target: | Others
Target Category: | Others
Method of detection: | Optical imaging
Source of signal / contrast: | Indotricarbocyanine (DiR)
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=molecular%20imaging%20and%20integrin%20%CE%B1v%CE%B23)]

Indotricarbocyanine (DiR)-loaded AS1411 DNA aptamer- and TGN peptide-modified poly(ethylene glycol)-poly(ε-caprolactone) (PEG-PCL) nanoparticles, abbreviated as DiR-AsTNP, is a cascade delivery system synthesized by Gao et al. for brain glioma imaging and treatment (1).

Effective treatment of brain tumors requires the therapeutic agents to penetrate both the blood–brain barrier (BBB) and the tumor cell barrier. The cascade targeting strategy is designed to meet this requirement, which relies on two specific ligands that are conjugated to a nanocarrier (1, 2). One ligand is designed to penetrate the BBB, and another is designed to target tumor tissues. With this strategy, Gao et al. developed a PEG-PCL cascade targeting delivery system that was modified with an angiopep-2 peptide to penetrate the BBB and an EGFP-EGF1 fusion protein to bind the brain neuroglial cells (2). Because of the promising results of this system, Gao et al. further developed another PEG-PCL system using TGN and AS1411 ligands (AsTNP) (1). TGN is a peptide of 12 amino acids (TGNYKALHPHNG), which was obtained through four rounds of in vivo phage display screening from a 12-mer peptide library (3). In vivo phage display is a technique that was first introduced by Pasqualini and Ruoslahti in 1996 (4). This technique has been used to screen tissue-specific peptides as targeting moieties for tumors and organs. The three-amino-acid sequence Arg-Gly-Asp is one of the most successful targeting ligands screened with the phage display technique (5). The TGN peptide has been shown to possess a superior BBB-penetrating ability compared with the native phage (3). AS1411 is a G-rich DNA aptamer that exhibits high binding affinity to nucleolin, a highly expressed protein in the plasma membrane of cancer cells including the C6 glioma cells (6, 7). Aptamers are short sequences of DNA or RNA that can bind to specific proteins via recognition of their three-dimensional structures (6). Aptamers are good candidates for targeted delivery because of their high stability, easy synthesis, and nonimmunogenicity (7). AS1411 has been used successfully to increase the anti-tumor efficacy of nanoparticles containing chemotherapeutic agents (7). In the AsTNP system, the TGN peptide served as the first-stage targeting ligand to transport the PEG-PCL nanoparticles through the BBB, and the AS1411 aptamer served as the second-stage ligand to deliver the system into the cancer cells after penetrating the BBB. An inhibitor of microtubule depolymerization, docetaxel (DTX), was then encapsulated within the AsTNP particles for therapeutic purpose (1, 8). A fluorescent dye (DiR or coumarin-6) was also encapsulated to track the behavior of AsTNP with optical imaging. The results obtained by Gao et al. showed that presence of both TGN and AS1411 was necessary, and the generated AsTNP had a superior BBB-penetration ability and high tumor accumulation (1). This chapter summarizes the data obtained with DiR-AsTNP.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=RAFT-RGD%20and%20imaging)]

Gao et al. described the synthesis of AsTNP and relevant nanoparticles in detail (1). The methoxy PEG-PCL (MPEG-PCL; molecular weight (MW), 3–15 kDa), R-carboxyl PEG-PCL (HOOC-PEG-PCL; MW, 3.4–15 kDa), and maleimide PEG-PCL (MAL-PEG-PCL; MW, 3.4–15 kDa) diblock copolymers were synthesized with ring-opening polymerization of the ε-caprolactone in dry toluene with MPEG, HOOC-PEG, or maleimide-PEG as the initiator and stannous octoate as the catalyst. The chemical structures of the three diblock copolymers were confirmed with ^1^H NMR. The MW of the MPEG-PCL, HOOC-PEG-PCL, and MAL-PEG-PCL was 14,947.6, 14,975.5, and 16,866.8 Da, respectively.

The PEG-PCL nanoparticles (designated as NP) were prepared with an emulsion/solvent evaporation method (1). The carboxyl unit of NP was then activated and conjugated with AS1411 through reaction for 4 h in the dark (designated as AsNP). Conjugation of TGN was achieved by reaction with NP (designated as TNP) or AsNP (designated as AsTNP) for 6 h in the dark. Sepharose CL-4B column was used to remove the free AS1411 and TGN. For imaging and therapeutic purposes, DTX-, coumarin-6-, and DiR-loaded nanoparticles were also prepared separately with similar procedures.

Gao et al. characterized the size, morphology, and zeta potential of this system (1). Dynamic light scattering revealed that NP, AsNP, AsTNP, and TNP had diameters of 151.6 nm, 162.8 nm, 170.6 nm, and 153.6 nm, respectively. Conjugation with AS1411 or TGN slightly increased the particle sizes, and encapsulation of DTX, coumarin-6, or DiR did not affect the particle size. Transmission electron microscopy showed that these particles were generally spheroid in shape. The zeta potential was approximately −4.45 mV, −8.91 mV, −8.79 mV, and −2.31 mV for NP, AsNP, AsTNP, and TNP, respectively. The negative charge of the AS1411 lowered the zeta potentials of the AsNP and AsTNP compared to that of the NP. The information on how many TGN or AS1411 were bound per NP was not provided.

Release of encapsulated coumarin-6 and DiR from the particles was evaluated with a dialysis method, and the results showed that the accumulated release of coumarin-6 and DiR from the particles was <0.1% of their total amounts within three days. The DTX encapsulation efficiency (DTX encapsulated/DTX total × 100%) and drug-loading capacity (DTX encapsulated/materials × 100%) were 47.8% and 1.59%, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19111043)]

In vitro cell uptake of the nanoparticles was evaluated with C6 glioma cells and bEnd.3 cells after incubation for 1 h with coumarin-6-loaded NP, AsNP, TNP, or AsTNP (1). bEnd.3 cells are an immortalized mouse brain endothelial cell line exhibiting endothelial properties. This cell line is widely used as a model of BBB due to its rapid growth, maintenance of the BBB characteristics over repeated passages, formation of functional barriers, and amenability to molecular interventions (9). Fluorescent microscopy showed that the uptake by both cell types was dependent on the particle formulations. For the bEnd.3 cells, the cellular uptake for AsNP was only slightly higher than that for NP, suggesting that AS1411 did not enhance the uptake by bEnd.3 cells. Conjugation with TGN markedly increased the cellular uptake for AsTNP and TNP, indicating that TGN effectively mediated the uptake of the nanoparticles by endothelial cells. For the C6 cells, the uptake of TNP was almost the same as that of NP, but the uptake of AsNP and AsTNP was higher than that of TNP and NP, which was considered to be due to the AS1411-mediated endocytosis. These results demonstrated that TGN mediated the first-stage targeting and AS1411 mediated the second-stage targeting.

The cellular uptake of the nanoparticles was further evaluated with tumor spheroids that were prepared by seeding C6 cells in low-melting-temperature agarose for 7 days (1). Confocal microscopy showed that AsNP and AsTNP distributed through the whole spheroids with high fluorescent intensity. In contrast, TNP and NP were only observed at the surface of C6 spheroids with weak fluorescence. These results indicate that AS1411 effectively increased the tumor cell uptake, but TGN did not.

Analysis with co-culture of the C6 spheroids with bEnd.3 monolayers showed that the co-culture significantly decreased the spheroid uptake of AsNP but not the uptake of AsTNP. Of the four formulations, AsTNP had the highest uptake and NP had the lowest. These results suggested that TGN enhanced the transport of nanoparticles across the bEnd.3 monolayer but did not increase their uptake by the C6 spheroids; both AS1411 and TGN were necessary for effective barrier penetration and cell uptake.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=RAFT-RGD%20and%20imaging)]

In vivo imaging was performed in C6 orthotopic glioma-bearing BALB/c nude mice after injection of the DiR-loaded NP, AsNP, TNP, or AsTNP (no description for the number of mice used) (1). NP and AsNP without TGN conjugation showed similar weak fluorescence in the mouse brain, although the tumor fluorescence intensity obtained from AsNP was 0.65-fold higher than that from NP, indicating that AS1411 did not enhance the brain uptake of the particles. On the contrary, TGN-conjugated TNP and AsTNP showed strong fluorescence in the brain, which reached the highest intensity at 12 h after injection. The fluorescent intensity in the brain for TNP and AsTNP was 3.76-fold and 1.38-fold higher, respectively, than that for NP. However, ex vivo imaging of the brain at 24 h after injection showed that TNP distributed throughout the whole brain without selectivity, while AsTNP mainly accumulated in the glioma of the brain, indicating effective tumor targeting with AS1411. The tumor uptake for AsTNP and TNP was 3.91-fold and 2.95-fold higher, respectively, than that for NP. The highest tumor/brain ratio was obtained with AsTNP, but this ratio obtained with TNP was lower than that with NP due to high brain fluorescence for TNP. These results indicated that conjugation with TGN and AS1411 enhanced the glioma uptake of the nanoparticles and increase the tumor/brain ratio in vivo.

In vivo anti-glioma efficacy of DTX-loaded AsTNP, AsNP, TNP, or NP was evaluated in C6 orthotopic glioma-bearing BALB/c nude mice after injection of 6 mg/kg of each formulation every three days for three times (n = 6 mice/group) (1). Saline and DTX were used as controls. Log-rank tests showed that the median survival times for the mice treated with AsNP, AsTNP, and TNP were all significantly longer than those of the mice treated with saline and DTX (Table 1). Treatment with AsTNP resulted in the longest survival time. In this study, AsNP also significantly increased the median survival time compared with NP, although the second-stage targeting ligand TGN was not conjugated. DTX and NP had no anti-glioma effect, similar to saline, which was most likely due to the low dose of DTX used in the experiment. These results demonstrated that combined TGN and AS1411 conjugation could enhance the anti-tumor efficacy of the nanoparticles.

Table 1: The median survival time of the mice bearing orthotropic glioma after treatment.

Group | Median (day) | 95% Confidence Interval | Significant | IST
Saline | 17.0 | 15.5–18.5
DTX | 18.0 | 14.4–21.6 | | 6%
NP | 17.0 | 13.8–20.2 | | 0%
AsNP | 25.0 | 20.2–29.8 | a, b, c | 47%
AsTNP | 32.0 | 26.0–38.0 | a, b, c, d, e | 88%
TNP | 25.0 | 13.0–37.0 | a, b | 47%

^a^P < 0.05 vs saline, ^b^P < 0.05 vs DTX, ^c^P < 0.05 vs NP, ^d^P < 0.05 vs AsNP, ^e^P < 0.05 vs TNP.

IST, increase in survival time compared with saline group.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Gao H., Qian J., Cao S., Yang Z., Pang Z., Pan S., Fan L., Xi Z., Jiang X., Zhang Q. (2012). Precise glioma targeting of and penetration by aptamer and peptide dual-functioned nanoparticles. Biomaterials.
2 Huile G., Shuaiqi P., Zhi Y., Shijie C., Chen C., Xinguo J., Shun S., Zhiqing P., Yu H. (2011). A cascade targeting strategy for brain neuroglial cells employing nanoparticles modified with angiopep-2 peptide and EGFP-EGF1 protein. Biomaterials.
3 Li J., Feng L., Fan L., Zha Y., Guo L., Zhang Q., Chen J., Pang Z., Wang Y., Jiang X., Yang V.C., Wen L. (2011). Targeting the brain with PEG-PLGA nanoparticles modified with phage-displayed peptides. Biomaterials.
4 Pasqualini R., Ruoslahti E. (1996). Organ targeting in vivo using phage display peptide libraries. Nature.
5 Gaertner F.C., Kessler H., Wester H.J., Schwaiger M., Beer A.J. (2012). Radiolabelled RGD peptides for imaging and therapy. Eur J Nucl Med Mol Imaging.
6 Teng Y., Girvan A.C., Casson L.K., Pierce W.M., Qian M., Thomas S.D., Bates P.J. (2007). AS1411 alters the localization of a complex containing protein arginine methyltransferase 5 and nucleolin. Cancer Res.
7 Guo J., Gao X., Su L., Xia H., Gu G., Pang Z., Jiang X., Yao L., Chen J., Chen H. (2011). Aptamer-functionalized PEG-PLGA nanoparticles for enhanced anti-glioma drug delivery. Biomaterials.
8 Xu Z., Chen L., Gu W., Gao Y., Lin L., Zhang Z., Xi Y., Li Y. (2009). The performance of docetaxel-loaded solid lipid nanoparticles targeted to hepatocellular carcinoma. Biomaterials.
9 Hu K., Li J., Shen Y., Lu W., Gao X., Zhang Q., Jiang X. (2009). Lactoferrin-conjugated PEG-PLA nanoparticles with improved brain delivery: in vitro and in vivo evaluations. J Control Release.